# N-[^11^C]Methylpiperidin-4-yl acetate

Chemical name: | N-[^11^C]Methylpiperidin-4-yl acetate
Abbreviated name: | [^11^C]MP4A, [^11^C]AMP
Synonym:
Agent category: | Compound
Target: | Acetylcholinesterase (AChE)
Target category: | Enzyme
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-Human Primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MP4A%5BAll%20Fields%5D)]

Acetylcholine is an endogenous neurotransmitter at cholinergic synapses and neuroneffector junctions in the peripheral and central nervous systems. It acts on nicotinic and muscarinic receptors to mediate complex functions, such as attention, memory, cognition, and consciousness. Degeneration of cholinergic neurons has been observed in several neurodegenerative disease, such as Alzheimer’s disease (AD) and Parkinson’s disease (PD), but not in vascular dementia. Acetylcholinesterase (AChE) is the enzyme that terminates cholinergic actions through the rapid hydrolysis of acetylcholine to choline and acetate. AChE is localized on both cholinergic and cholinoceptive neurons in the brain, with the highest activity in the striatum, thalamus, cerebellum, and cerebral cortex (1). AChE has been a target for radioligand development as well as drug development because its levels decrease in AD (1, 2). Radiolabeled AChE inhibitors and acetylcholine analog substrates are the two major approaches to mapping AChE in vivo in the human brain.

For measurements of AChE activity, various labeled esters of 1-methy-4-hydroxypiperidine have been designed and evaluated as acetylcholine substrate analogs (3). One of these analogs, N-[^11^C]methylpiperidin-4-yl acetate ([^11^C]MP4A), was chosen for further development as a positron emission tomography (PET) radioligand. It has a tertiary amine structure that makes it lipophilic, and thus it readily crosses the blood-brain barrier (BBB). [^11^C]MP4A is specifically hydrolyzed by AChE (99% specificity) and yields a hydrophilic metabolite, N-[^11^C]methylpiperidinol ([^11^C]MP4OH), which is trapped in the brain because it is too polar to cross the BBB. [^11^C]MP4A is being developed as a PET agent for the non-invasive study of brain AChE activity in patients with AD and PD.

### Related Resource Links

- Chapters in MICAD (AChE (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=acetylcholinesterase++AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (AChE (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=43&log$=genesensor5&logdbfrom=protein)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=cholinesterase) (AChE (http://omim.org/entry/100740))
- Clinical trials (AChE (http://www.clinicaltrials.gov/ct2/results?term=acetylcholinesterase))
- Drug information in FDA (AChE (http://google-test.fda.gov/search?q=Acetylcholinesterase+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=15&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MP4A%20and%20synthesis)]

Irie et al. (3) reported the synthesis of [^14^C]MP4A by direct N-methylation of piperidin-4-yl acetate with [^14^C]methyl iodine in acetone, with a radiochemical yield of 80% (end of synthesis) after purification via high-performance liquid chromatography. Radiochemical purities were >97% with a total synthesis time of ~30 min. Iyo et al. (4) reported a specific activity of 18 GBq/μmol (0.49 Ci/μmol) when they used this same method to prepare [^11^C]MP4A . Nguyen et al. (5) prepared [^11^C]MP4A using [^11^C]methyl triflate for N-methylation in dimethyl sulfoxide, with radiochemical yields of 10-40%. Carpinelli et al. (6) described a fully automated synthesis of [^11^C]MP4A using [^11^C]methyl iodine for N-methylation of piperidin-4-yl acetate hydrochloride in anhydrous dimethylformamide; the radiochemical purity of the product was >98%. The radiochemical yields were 20-60% within 40 min after end of bombardment, with an average specific activity of 37 GBq/μmol (1 Ci/μmol) (n = 10).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MP4A%20and%20in%20vitro)]

Irie et al. (7) reported that MP4A was rapidly hydrolyzed to MP4OH and acetic acid by mouse, rat, and human brain homogenates, with 94-99% specificity for AChE. The hydrolysis rate in human cerebral cortex (0.16/fraction/min/g/ml) is about 10% of that in the cerebral cortex of the rat and mouse (1.54/fraction/min/g/ml).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MP4A%20and%20rodentia)]

Biodistribution studies by Irie et al. (7) in mice showed rapid, high accumulation of radioactivity in the brain within minutes after injection of [^14^C]MP4A. The uptakes in striatum, cortex, and cerebellum were about 10% of injected dose/g at 1 min, and >95% of radioactivity was the hydrolytic metabolite, [^14^C]MP4OH. There was little difference in regional blood flow measured by [^123^I]isopropyliodoamphetamine ([^123^I]IMP). In contrast, [^14^C]MP4A showed heterogeneous distributions, with striatum/cerebellum and cortex/cerebellum ratios of 2.1-3.8 and 1.4-2.0, respectively.

Kilbourn et al. (8) reported that 30 min after injection in mice, [^11^C]MP4A showed rapid accumulation in the brain and a regional retention of radioactivity (striatum > cortex, hippocampus > hypothalamus > cerebellum) reflecting known levels of AChE activity in the brain, with >95% of radioactivity in the form of [^11^C]MP4OH. Striatum/cerebellum and striatum/cortex ratios were 1.94 ± 0.16 and 1.03 ± 0.14, respectively. Retention of radioactivity in all regions was reduced by pretreatment with 3 mg/kg diisopropylfluorophosphate (DFP), a specific irreversible AChE inhibitor. DFP treatment also significantly increased the proportions of intact ester in both the blood and brain.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MP4A%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MP4A%20and%20%28primate%20not%20human%29)]

Tsukada et al. (9) performed PET studies with [^11^C]MP4A in 5 young (5.2 ± 1.1 years old) and 5 aged (20.3 ± 2.6 years old) male rhesus monkeys and found rapid accumulation in the brain within minutes after injection. The highest uptake was in the striatum and thalamus, followed by the cerebellum, occipital cortex, temporal cortex, and frontal cortex. Quantitative analysis of [^11^C]MP4A uptake was usually described by a three-compartment model with three parameters to measure AChE activity (k_3_) with or without blood sampling. The striatum or cerebellum, used as a “reference region” because of their high AChE activity, reflected a biologic integrator of plasma input function during PET scanning. Donepezil (AChE inhibitor) at doses of 50 and 250 μg/kg suppressed the AChE activity (k_3_) of [^11^C]MP4A in all cortical regions in a dose-dependent manner in both age groups. However, the suppression was greater in young than in aged monkeys. AChE inhibition by donepezil led to a dose-dependent increase in acetylcholine levels in the prefrontal cortex of young animals as measured by microdialysis. Aged monkeys showed impaired working memory performance compared with young monkeys, and the impaired performance was partly improved by the administration of donepezil because of facilitation of the cholinergic neuronal system by AChE inhibition.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MP4A%20and%20human)]

Kinetic analysis of [^11^C]MP4A for measurement of cerebral AChE activity can be performed with or without arterial blood sampling (10-13). A three-compartment model with three parameters is used to measure AChE hydrolysis of the tracer (k_3_), the transport rate constant of the tracer from blood to brain through the BBB (K_1_), and the transport rate constant of the tracer from brain to blood through the BBB (k_2_). Using [^11^C]MP4A PET, Iyo et al. (4) studied eight elderly healthy controls and five patients with AD who had mild dementia. The estimated AChE distribution in the brain of the control subjects agreed with the AChE distribution at biopsy. The median K_1_ and k_2_ values for all regions in the controls were 0.54 ± 0.10 ml/g/min and 0.13 ± 0.02/min, respectively. The median K_1_ and k_2_ values in the AD patients were 0.42 ± 0.07ml/g/min and 0.11 ± 0.02/min, respectively. This reduction is attributable to the cortical reduction of regional blood flow in the AD patients as measured by [^123^I]IMP. All patients with AD had multiple cortical regions with a reduced k_3_ value compared with controls. The reduction in k_3_ was heterogeneous both regionally and individually. The reduction was more marked in the temporoparietal cortex, with an average reduction rate of 31% in the temporal and 38% in the parietal cortex, with less pronounced reductions in other cortical lesions (19% in the frontal, 24% in the occipital, and 20% in the sensorimotor cortex). Each patient was found to have at least two cortical regions with significantly reduced AChE activity.

Shinotoh et al. (14) subsequently confirmed a significant reduction in k_3_ values in the neocortex, hippocampus, and amygdale in 15 early-onset AD patients, whereas k_3_ values were significantly reduced only in the temporoparietal cortex and amygdale in late-onset AD patients. There was a significant correlation between the cortical k_3_ values and the Mini-Mental State Examination scores. Herholz et al. (15) found that AChE activity was significantly reduced in the amygdale and cerebral cortex in patients with mild to moderate AD, whereas reduction of cerebral blood flow and glucose metabolism was more limited to temporoparietal regions. Rinne et al. (16) cautioned that the k_3_ values in the hippocampus were only slightly reduced in mild cognitive impairment and early AD compared with AD, limiting their usefulness in detecting early AD.

Hilker et al. (17) performed combined PET with [^11^C]MP4A and [^18^F]fluorodopa (FDOPA) for evaluation of cholinergic and dopaminergic transmitter changes in 17 non-demented patients with PD and 10 PD patients with associated dementia (PDD) compared with 31 age-matched controls. The striatal FDOPA uptake was significantly decreased in PD and PDD without differences between the groups. The global cortical k_3_ values for [^11^C]MP4A were strongly reduced in PDD (29.7%; P < 0.001) and moderately decreased in PD (10.7%; P < 0.01) compared with controls. The PDD group had lower parietal k_3_ values for [^11^C]MP4A than did patients with PD. Frontal and temporoparietal cortices showed a significant correlation of striatal FDOPA reduction and decreased k_3_ for [^11^C]MP4A in patients with PDD.

Internal dosimetry data for [^11^C]MP4A in humans have not yet been available in the literature.

## References

1 Shinotoh H., Fukushi K., Nagatsuka S., Irie T. (2004). Acetylcholinesterase imaging: its use in therapy evaluation and drug design. Curr Pharm Des.
2 Herholz K. (2003). PET studies in dementia. Ann Nucl Med.
3 Irie T., Fukushi K., Akimoto Y., Tamagami H., Nozaki T. (1994). Design and evaluation of radioactive acetylcholine analogs for mapping brain acetylcholinesterase (AchE) in vivo. Nucl Med Biol.
4 Iyo M., Namba H., Fukushi K., Shinotoh H., Nagatsuka S., Suhara T., Sudo Y., Suzuki K., Irie T. (1997). Measurement of acetylcholinesterase by positron emission tomography in the brains of healthy controls and patients with Alzheimer's disease. Lancet.
5 Nguyen T.B., Snyder S.E., Kilbourn M.R. (1998). Syntheses of carbon-11 labeled piperidine esters as potential in vivo substrates for acetylcholinesterase. Nucl Med Biol.
6 Carpinelli A., Magni F., Cattaneo A., Matarrese M., Turolla E., Todde S., Bosso N., Galli Kienle M., Fazio F. (2006). Improved synthesis and radiolabeling of [11C]MP4A, a suitable ligand for the investigation of the cholinergic system using PET. Appl Radiat Isot.
7 Irie T., Fukushi K., Namba H., Iyo M., Tamagami H., Nagatsuka S., Ikota N. (1996). Brain acetylcholinesterase activity: validation of a PET tracer in a rat model of Alzheimer's disease. J Nucl Med.
8 Kilbourn M.R., Nguyen T.B., Snyder S.E., Sherman P. (1998). N-[11C]methylpiperidine esters as acetylcholinesterase substrates: an in vivo structure-reactivity study. Nucl Med Biol.
9 Tsukada H., Nishiyama S., Fukumoto D., Ohba H., Sato K., Kakiuchi T. (2004). Effects of acute acetylcholinesterase inhibition on the cerebral cholinergic neuronal system and cognitive function: Functional imaging of the conscious monkey brain using animal PET in combination with microdialysis. Synapse.
10 Herholz K., Lercher M., Wienhard K., Bauer B., Lenz O., Heiss W.D. (2001). PET measurement of cerebral acetylcholine esterase activity without blood sampling. Eur J Nucl Med.
11 Nagatsuka Si S., Fukushi K., Shinotoh H., Namba H., Iyo M., Tanaka N., Aotsuka A., Ota T., Tanada S., Irie T. (2001). Kinetic analysis of [(11)C]MP4A using a high-radioactivity brain region that represents an integrated input function for measurement of cerebral acetylcholinesterase activity without arterial blood sampling. J Cereb Blood Flow Metab.
12 Namba H., Fukushi K., Nagatsuka S., Iyo M., Shinotoh H., Tanada S., Irie T. (2002). Positron emission tomography: quantitative measurement of brain acetylcholinesterase activity using radiolabeled substrates. Methods.
13 Tanaka N., Fukushi K., Shinotoh H., Nagatsuka S., Namba H., Iyo M., Aotsuka A., Ota T., Tanada S., Irie T. (2001). Positron emission tomographic measurement of brain acetylcholinesterase activity using N-[(11)C]methylpiperidin-4-yl acetate without arterial blood sampling: methodology of shape analysis and its diagnostic power for Alzheimer's disease. J Cereb Blood Flow Metab.
14 Shinotoh H., Namba H., Fukushi K., Nagatsuka S., Tanaka N., Aotsuka A., Ota T., Tanada S., Irie T. (2000). Progressive loss of cortical acetylcholinesterase activity in association with cognitive decline in Alzheimer's disease: a positron emission tomography study. Ann Neurol.
15 Herholz K., Weisenbach S., Zundorf G., Lenz O., Schroder H., Bauer B., Kalbe E., Heiss W.D. (2004). In vivo study of acetylcholine esterase in basal forebrain, amygdala, and cortex in mild to moderate Alzheimer disease. Neuroimage.
16 Rinne J.O., Kaasinen V., Jarvenpaa T., Nagren K., Roivainen A., Yu M., Oikonen V., Kurki T. (2003). Brain acetylcholinesterase activity in mild cognitive impairment and early Alzheimer's disease. J Neurol Neurosurg Psychiatry.
17 Hilker R., Thomas A.V., Klein J.C., Weisenbach S., Kalbe E., Burghaus L., Jacobs A.H., Herholz K., Heiss W.D. (2005). Dementia in Parkinson disease: functional imaging of cholinergic and dopaminergic pathways. Neurology.